# ^89^Zr-Labeled anti-CD105 (endoglin) chimeric monoclonal antibody TRC105 linked to IRDye 800CW

Chemical name: | ^89^Zr-Labeled anti-CD105 (endoglin) chimeric monoclonal antibody TRC105 linked to IRDye 800CW
Abbreviated name: | [^89^Zr]TRC105-IRDye800CW
Synonym:
Agent Category: | Antibody
Target: | CD105 (endoglin) antigen
Target Category: | Antigen
Method of detection: | Multimodal (positron emission tomography (PET); fluorescence optical imaging)
Source of signal / contrast: | ^89^Zr (PET); IRDye800CW (fluorescence optical imaging)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD105&cmd=DetailsSearch)]

The CD105 antigen (endoglin) is a hypoxia-inducible, 180-kDa, disulfide-linked, homodimeric transmembrane glycoprotein that is a co-receptor for the transforming growth factor β (TGF-β) (1). Both CD105 and TGF-β are expressed at low levels in resting endothelial cells, but they are overexpressed in cancerous lesions and play a significantly proangiogenic role in remodeling the vasculature of malignant tumors (2). It has been shown that the levels of CD105 in endothelial tissues correlate well with the degree of cell proliferation. In addition, the antigen has been found to be a suitable biomarker to quantify tumor angiogenesis and can be used to determine the prognostic outcome for cancer patients (3). The biological activity of CD105 has been discussed in detail by Seon et al. (4). Investigators have demonstrated that immunotoxins and radioimmunoconjugates generated with anti-CD105 monoclonal antibodies (mAbs) can inhibit angiogenesis and prevent the growth and metastasis of cancerous tumors (4). For translation to the clinic, a human/mouse chimeric anti-CD105 mAb (designated c-SNj6 or TRC105) was generated and shown to have suitable pharmacokinetic, toxicological, and immunogenicity characteristics for use in non-human primates (5). Currently, a clinical trial (http://clinicaltrials.gov/ct2/show/NCT01326481?term=endoglin&rank=5) is in progress to evaluate the use of TRC105 for the treatment of metastatic breast cancer.

TRC105 was labeled with ^64^Cu (6) and ^89^Zr (7), respectively, and has been reported to detect the expression of CD105 with positron emission tomography (PET) imaging in xenograft tumors in mice. In another study, TRC105 was conjugated to IRDye 800CW, a near-infrared fluorescent (NIRF) dye, and the expression of CD105 in tumors was visualized with NIRF imaging (8). TRC105 has also been conjugated with ^64^Cu and IRDye 800CW to develop a dual-modality (PET/NIRF) imaging agent that can be used to detect murine breast cancer 4T1cell tumors in mice (9). Recently, TRC105 was conjugated to 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA) and labeled with ^66^Ga, and the radioimmunoconjugate was shown to be suitable for the visualization of CD105 expression with PET in 4T1 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) xenograft tumors in mice (10).

In a proof-of-principle study, the biodistribution of ^66^Ga-labeled NOTA covalently linked to a sheet of PEGylated nano-graphine (GO) conjugated to TRC105 ([^66^Ga]-NOTA-GO-TRC105) was investigated in mice bearing 4T1 cell xenograft tumors. It was shown that the labeled mAb conjugate was suitable for use with PET imaging to visualize CD105-positive tumors (11). In another study with the same tumor model, it was demonstrated that [^64^Cu]-NOTA-GO-TRC105 can be used to visualize the CD105-positive lesions in rodents (12).

However, there are limitations to using a single imaging modality for the visualization of cancerous lesions (e.g., PET is very sensitive, but it has a low resolution; although optical imaging is inexpensive and easy to use, it cannot be used to quantify a target accurately with external imaging) (13, 14). In an effort to improve the applications of a targeted imaging agent, investigators suggested that combining the PET and fluorescence imaging modalities within a single imaging agent may be advantageous compared with the use of either modality alone (13, 14). While PET can be used to locate and quantify a target, NIRF imaging can be used to visualize and resect the target-bearing lesions during surgery (13, 14). With this in mind, TRC105 was labeled with ^89^Zr and linked to IRDye 800CW (emission maxima 806 nm; [^89^Zr]TRC105-IRDye 800CW), and the dual-labeled mAb was evaluated for the imaging of tumor angiogenesis in mice bearing either fLuc-4T1 cell tumors (these 4T1 cells were transfected with the firefly luciferase) (13) or 4T1 cell tumors (14). The biodistribution of [^89^Zr]TRC105-IRDye 800CW was also investigated in rodents bearing tumors of either cell type (13, 14).

### Related Resource Links

TRC105 (http://www.ncbi.nlm.nih.gov/books/?term=TRC105+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Other anti-CD105 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-CD105+antibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD105 (endoglin) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/BC014271.2) sequences

CD105 gene information (http://www.ncbi.nlm.nih.gov/gene/2022) (Gene ID: 2022)

CD105 in Online Mendelian Inheritance in Man Database (http://omim.org/entry/131195) (OMIM)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=TRC105) related to TRC105

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B89Zr%5DTRC105%20IRDye800CW%20synthesis&cmd=DetailsSearch)]

The synthesis of [^89^Zr]TRC105-IRDye 800CW has been described elsewhere (13, 14). Briefly, a bifunctional chelating agent, p-isothiocyanatobenzyl-desferrioxamine B (Df; to bind the radionuclide), and IRDye 800CW were separately conjugated to TRC105, and the conjugated mAb was subsequently radiolabeled with ^89^Zr. For use as a control, [^89^Zr]cetuximab-IRDye 800CW (cetuximab binds to the epidermal growth factor receptor and does not target the CD105 antigen) was also prepared with the same procedures (13, 14). Approximately 1.0 molecule of Df and 0.9 molecule of IRDye 800CW were reported to be conjugated to each molecule of TRC105 and cetuximab as determined with ultraviolet measurements (13). In a second study, ~0.6 molecule of Df and 0.7 molecule of IRDye 800CW were reported to be conjugated to each molecule of TRC105 and cetuximab (14).

The radiochemical yield (RCY) of each ^89^Zr-labeled mAb was 55 ± 14% (the radiochemical purity (RCP) was not reported), and each labeled mAb had a specific activity (SA) of ~80 MBq/mg (2.16 mCi/mg) (13). In another study, the RCY and RCP of the two ^89^Zr-labeled mAbs were 55 ± 10% and >95%, respectively, and the SA of both labeled mAbs were 0.08–0.4 GBq/mg (2.16–10.81 mCi/mg) (14). In both studies, the time taken to label and purify the ^89^Zr-labeled mAbs was 100 ± 10 min (13, 14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TRC105%20in%20vitro&cmd=DetailsSearch)]

The immunoreactivity of TRC105 and Df-TRC105-800CW was compared with fluorescence-activated cell sorting (FACS) analysis using HUVEC cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) (express >10^6^ CD105 per cell) and MCF-7 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) (do not express CD105) (13). Both TRC105 and Df-TRC105-800CW showed a similar binding to HUVEC cells, and neither mAb showed any binding to the MCF-7 cells (13). Similar results were reported by Zhang et al. (14).

The stability values of [^89^Zr]TRC105-IRDye 800CW and [^89^Zr]cetuximab-IRDye 800CW were not reported (13, 14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TRC105%20rodentia&cmd=DetailsSearch)]

fLuc-4T1 cell tumors were generated in the lungs of mice (n = 8 animals), and development of lesions in the animals was monitored with bioluminescence imaging (BLI) on different days after intraperitoneal injection of D-luciferin (13). A sufficiently strong BLI signal was detected in the lungs of the rodents at ~21 d after inoculation of the fLuc-4T1 cells, and the animals were subsequently used for the biodistribution and PET/NIRF imaging studies (13).

For PET imaging and biodistribution studies, the animals (n = 4 mice/time point) were injected with 5–10 MBq (135.1–170.2 μCi) of the tracer through the tail vein, and whole-body PET images of the mice were acquired at time points ranging from 4 h postinjection (p.i.) to 48 h p.i. The images showed that at 4 h p.i. the radioactivity from [^89^Zr]TRC105-IRDye 800CW was present mainly in the blood. At 24 h p.i., the lung tumors were visible; at 48 h p.i., multiple lesions could be seen very clearly in these organs. Region-of-interest analysis of the PET images was used to calculate the amount of radioactivity accumulated in the blood, liver, and lung tumors of the animals. Data generated from this analysis were presented as percent of injected dose per gram tissue (% ID/g; Table 1)).

Table 1: Accumulation of radioactivity in blood, liver, and lung tumors of animals injected with [ ^ 89 ^ Zr]TRC105-IRDye 800CW alone or in animals injected with a blocking dose (13.33 nmol) of nonradioactive TRC105 2 h before injection of the tracer ( 13 ).

Tissues | Accumulation of radioactivity at different time points postinjection
Tissues | 4 h | 24 h | 48 h
Blood | 14.7 ± 1.5 | 7.9 ± 0.6 | 7.4 ± 1.1
Liver | 18.3 ± 1.7 (19.5 ± 2.7)* | 16.8 ± 2.2 (17.8 ± 1.2)* | 16.2 ± 2.2 (17.5 ± 0.7)*
Tumors | 8.7 ± 1.4 (4.2 ± 0.4)*# | 10.9 ± 0.5 (4.9 ± 0.5)*# | 9.7 ± 1.1 (4.9 ± 0.3)*#

*Numbers in parenthesis show accumulated radioactivity in tissues of animals given a blocking dose of nonradioactive TRC105. #, P < 0.01.

Table 1 shows that there was a statistically significant reduction (P < 0.01) in accumulation of radioactivity in the tumors of animals pre-injected with a blocking dose of nonradioactive TRC105. However, no such change was apparent in the liver of animals with or without the blocking dose (Table 1). In addition, the amount of radioactivity taken up by the tumors of animals (n = 4 mice) injected with [^89^Zr]-cetuximab-IRDye 800CW was 4.3 ± 0.6% ID/g, 4.2 ± 0.3% ID/g, and 4.9 ± 0.3% ID/g at 4 h p.i., 24 h p.i., and 48 h p.i., respectively, which was significantly lower (P < 0.01) than the uptake observed with [^89^Zr]TRC105-IRDye 800CW in the lesions (13). From these observations, the investigators concluded that [^89^Zr]TRC105-IRDye 800CW had a high binding specificity for CD105 expressed in the tumors (13).

After the final PET scan at 48 h p.i., the animals were euthanized and the major organs were removed for ex vivo BLI, NIRF, and PET imaging (13). With all imaging modalities, maximum signal was observed in the liver, followed by the tumors, and all the other organs exhibited lower levels of the signal with all the imaging modalities. The different imaging modalities generated a similar amount of signal with [^89^Zr]TRC105-IRDye 800CW and [^89^Zr]-cetuximab-IRDye 800CW, respectively, in all the organs except in the tumor-bearing lungs. In addition, the uptake of label from [^89^Zr]TRC105-IRDye 800CW in the tumors of the blocked animals was significantly lower (P < 0.01) than in the lesions of the test animals.

Ex vivo immunofluorescence co-staining of the different tissues for CD105 and CD31 showed that the CD105 antigen was expressed primarily in the vasculature of the lung tumors. In addition, the level of CD105 expression in the lesion-bearing lungs was higher than that observed in the normal lungs (13). A low level of CD105 staining was observed in the liver and kidneys of the tumor-bearing animals, suggesting that the uptake of radioactivity in these tissues was primarily due to non-specific binding and uptake by the reticuloendothelial system, and that clearance of the tracer from the system was primarily through the hepatobiliary route (13).

Zhang et al. investigated the biodistribution and multimodal imaging properties of [^89^Zr]TRC105-IRDye 800CW and [^89^Zr]-cetuximab-IRDye 800CW in the same mouse model described above (14). Results obtained by Zhang et al. were similar to those detailed above; therefore, the experimental procedures and data of this investigation will not be discussed here. Readers interested in the biodistribution and imaging data generated by Zhang et al. should consult the original publication (14).

From these studies, the investigators concluded that dual-labeled PET/NIRF imaging agents can probably be used for the noninvasive detection and imaging-guided surgery of diseased tissues (13, 14). However, further development and optimization of the dual-labeled tracers is necessary before they can be used in the clinic (13, 14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TRC105%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TRC105%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TRC105%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Parts of the studies mentioned in this chapter were supported by a National Institutes of Health grant through the UW Radiological Sciences Training Program 5 T32 CA009206-32.

## References

1 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
2 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
3 Fonsatti E., Nicolay H.J., Altomonte M., Covre A., Maio M. (2010). Targeting cancer vasculature via endoglin/CD105: a novel antibody-based diagnostic and therapeutic strategy in solid tumours. Cardiovasc Res.
4 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
5 Shiozaki K., Harada N., Greco W.R., Haba A., Uneda S., Tsai H., Seon B.K. (2006). Antiangiogenic chimeric anti-endoglin (CD105) antibody: pharmacokinetics and immunogenicity in nonhuman primates and effects of doxorubicin. Cancer Immunol Immunother.
6 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
7 Hong H., Severin G.W., Yang Y., Engle J.W., Zhang Y., Barnhart T.E., Liu G., Leigh B.R., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of CD105 expression with 89Zr-Df-TRC105. Eur J Nucl Med Mol Imaging.
8 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
9 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Optical Imaging of Tumor CD105 Expression with a Dual-Labeled Monoclonal Antibody. Mol Pharm.
10 Engle J.W., Hong H., Zhang Y., Valdovinos H.F., Myklejord D.V., Barnhart T.E., Theuer C.P., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of tumor angiogenesis with a (66)ga-labeled monoclonal antibody. Mol Pharm.
11 Hong H., Zhang Y., Engle J.W., Nayak T.R., Theuer C.P., Nickles R.J., Barnhart T.E., Cai W. (2012). In vivo targeting and positron emission tomography imaging of tumor vasculature with (66)Ga-labeled nano-graphene. Biomaterials.
12 Hong H., Yang K., Zhang Y., Engle J.W., Feng L., Yang Y., Nayak T.R., Goel S., Bean J., Theuer C.P., Barnhart T.E., Liu Z., Cai W. (2012). In vivo targeting and imaging of tumor vasculature with radiolabeled, antibody-conjugated nanographene. ACS Nano.
13 Hong, H., Y. Zhang, G.W. Severin, Y. Yang, J.W. Engle, G. Niu, R.J. Nickles, X. Chen, B.R. Leigh, T.E. Barnhart, and W. Cai, Multimodality Imaging of Breast Cancer Experimental Lung Metastasis with Bioluminescence and a Monoclonal Antibody Dual-Labeled with (89)Zr and IRDye 800CW. Mol Pharm, 2012
14 Zhang Y., Hong H., Severin G.W., Engle J.W., Yang Y., Goel S., Nathanson A.J., Liu G., Nickles R.J., Leigh B.R., Barnhart T.E., Cai W. (2012). ImmunoPET and near-infrared fluorescence imaging of CD105 expression using a monoclonal antibody dual-labeled with (89)Zr and IRDye 800CW. Am J Transl Res.